# Self-quenching Alexa fluor 680 conjugated to trastuzumab

Chemical name: | Self-quenching Alexa fluor 680 conjugated to trastuzumab
Abbreviated name: | Tra-Alexa680(SQ)
Synonym:
Agent Category: | Humanized monoclonal antibody
Target: | Epidermal growth factor receptor 2 (HER2)
Target Category: | Receptor
Method of detection: | Optical imaging: fluorescence
Source of signal / contrast: | Alexa fluor 680
Activation: | Yes
Studies: | - In vitro; - Rodents | Click here for information regarding human EGFR (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=gene&Cmd=retrieve&dopt=full_report&list_uids=1956&log$=databasead&logdbfrom=protein).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=alexa+680+conjugated+to+trastuzumab)]

Humanized monoclonal antibodies (MAbs) conjugated to radionuclides used for the detection and treatment of cancers have limited efficacy because they are large glycoprotein molecules (~150 kD) that cannot penetrate deep into cancerous tumors (1). In general, radioimmunoconjugates, including those used for imaging purposes, have a prolonged blood circulation and, if used for radioimmunotherapy ( high-energy β-emitters such as yttrium or rhenium, etc., or α-emitters such as bismuth or astatine, etc.), can impair the functioning of normal cells and may be myelotoxic (1). The use and limitations of radioimmunoconjugates as imaging and therapeutic agents were discussed in detail by Sharkey and Goldenberg (1). As an alternative to using radionuclides in conjunction with MAbs for the detection of cancer, investigators have explored the use of fluorescent agent-MAbs and other molecule conjugates for the preclinical imaging of cancerous tumors (2-6). However, the fluorescent dye-MAb probes, although cheap to generate, have blood circulation and tumor penetration drawbacks similar to the radioimmunoconjugates and also exhibit a high background because of autofluorescence generated in the tissue (6, 7). To circumvent problems observed with the optical probes, investigators have generated self-quenching, targeted fluorescent dye-MAb conjugates that are non-fluorescent in the native state but generate a signal only when activated by degradation of the targeting MAb or molecule by a specific cellular process or organelle (8). Accumulation of the fluorescent dye within a target cell would reduce the non-specific background and decrease the blood pool signal.

The chemical structure of self-quenching probes is such that a quencher molecule is closely associated in alignment with the fluorophore. Enzymatic cleavage of the structure results in separation of the quencher from the fluorophore and in the generation of a fluorescent signal (8). Near-infrared (NIR) probes such as Alexa fluor and Cy5.5 are favored over other optical agents because they exhibit superior tissue penetration (hemoglobin and water have low absorption of the NIR signal at the operating wavelengths of these probes), and when two or more NIR probe molecules are conjugated, the fluorescent signal quenches itself. Cleavage of the conjugation bonds results in fluorescence dequenching and generation of a signal that is suitable for imaging (9-11). However, it is pertinent to mention that only a specific number of the NIR probe molecules can be conjugated to a macromolecule without changing the structural and pharmacokinetic properties of the macromolecule. Ogawa et al. conjugated multiple copies of Alexa fluor 680 (Alexa680) to trastuzumab (Tra), a humanized MAb that specifically targets the human epidermal growth factor receptor 2 (HER2), to synthesize a self-quenching, targeted NIR probe (Tra-Alexa680(SQ)) (12). Tra is approved (http://www.herceptin.com/index.jsp?s_cid=0001&s_src=googleppc&segmentID=1530&gclid=CPmJ952fj5kCFQu-Ggod1FuMbQ) by the United States Food and Drug Administration for use as a single agent or an adjuvant to treat certain types of breast cancer and is being tested in clinical trials (http://clinicaltrials.gov/ct2/results?term=trastuzumab) for the treatment of other neoplasms in humans. A characteristic feature of HER2 is that, upon binding a ligand, including the MAb directed against it, the receptor-ligand complex is internalized by the cell for enzymatic digestion in the lysosomes (13, 14). Proteolytic digestion of the receptor and the bound MAb in the lysosome releases the quencher from the fluorophore, resulting in generation of a signal. Therefore, a fluorophore that is “off” in the extracellular environment is turned “on” in an intracellular location. Ogawa et al. investigated the receptor specificity of Tra-Alexa680(SQ) under in vitro conditions using NIH-3T3 cells transfected with the HER2 gene (3T3/HER2^+^ cells), and to study the in vivo characteristics of the fluorophore-MAb conjugate the investigators used nude mice bearing xenograft and orthotropic tumors generated with 3T3/HER2^+^ or BALB/3T3/HER2^-^ cells (12).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20synthesis)]

Synthesis of the self-quenching Tra-Alexa680(SQ) conjugate was detailed by Ogawa et al. (12). Alexa680 (as a N-hydroxysuccinimide ester) and Tra were obtained from commercial sources. Briefly, the Tra-Alexa680(SQ) conjugate was synthesized by incubating Tra with Alexa680 in phosphate buffer (pH 8.5) for 30 min at room temperature. The conjugate was purified on a Sephadex G50 column and stored at 4°C as a stock solution. Approximately seven Alexa680 molecules conjugated to each MAb molecule, as determined with absorption on a UV-Vis spectrophotometric system.

A control “always on” conjugate, Tra-Alexa680(ON), was also synthesized, purified, and stored as above. The Tra-Alexa680(ON) conjugate was reported to have approximately one Alexa680 molecule per Tra molecule, as determined above (12).

The yield, purity, and stability of either conjugate, after purification, was not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20in%20vitro)]

Ogawa et al. used a fluorescence spectrometer to investigate the fluorescence quenching ability of the Tra-Alexa680 conjugates by exposing them to 5% sodium dodecyl sulfate and 1% 2-mercaptoethanol in phosphate-buffered saline for 2 min at 95°C (12). The quenching capacities of Tra-Alexa680(SQ) and Tra-Alexa680(ON) were reported to be 8- and 2-fold, respectively compared to the native (undenatured),self quenching, molecules (12).

The in vitro binding specificity of the Tra-Alexa680 conjugates was studied with the use of 3T3/HER2^+^ and the control BALB/3T3(HER2^-^) cells as described by Ogawa et al. (12). The two cell types were exposed to Tra-Alexa680 conjugates and viewed under a fluorescent microscope after 1 and 8 h. At 1 h, cell surface fluorescence was observed only on the 3T3/HER2^+^ cells, and at 8 h the fluorescence was emitted by fluorescent dots located inside the cells. A higher fluorescent signal was reported for cells treated with Tra-Alexa680(SQ) than for those treated with Tra-Alexa680(ON). A fluorescent signal due to Tra-Alexa680(ON) binding or internalization was not observed with the BALB/3T3/ZsGreen/HER2^-^ cells (these cells were transfected with the green fluorescent protein gene) when exposed respectively to either conjugate. This indicated that the two Tra-Alexa680 conjugates were bound to, and internalized by, only the HER2^+^ cells.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=alexa+680+conjugated+to+trastuzumab+rodentia)]

In vivo and ex vivo imaging studies performed with nude mice bearing 3T3/HER2^+^ and BALB/3T3/ZsGreen/HER2^-^ cell tumors were described by Ogawa et al. (12). The mice were injected with either Tra-Alexa680(SQ) or Tra-Alexa680(ON), respectively (number of animals used per conjugate was not reported), and imaging was performed 2 d after administration of the conjugates. Whole-body imaging of the animals revealed that the 3T3/HER2^+^ tumor images were much more enhanced compared to those generated with the BALB/3T3/ZsGreen/HER2^-^ cells. Also, with Tra-Alexa680(ON), the fluorescent signal was obtained not only from the HER2^+^ cells but also from the HER2^-^ cells, although the signal generated from the latter cells was considerably lower. Ex vivo imaging of the tumors yielded results similar to those obtained during the whole-body imaging studies (12). In addition, the fluorescent signal obtained from the blood pool was reported to be low with Tra-Alexa680(SQ) compared with Tra-Alexa680(ON). Similar results were also reported with animals bearing 3T3/HER2^+^ and BALB/3T3/ZsGreen/HER2^-^ cell orthotropic tumors (12).

With results obtained from this study, the investigators concluded that it is possible to apply this technology to other humanized MAbs of the immunoglobulin G_1_ class for the development of targeted imaging agents (12).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=alexa+680+conjugated+to+trastuzumab+Non+Primate+Mammals)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=alexa+680+conjugated+to+trastuzumab+Non+Human+Primates)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=alexa+680+conjugated+to+trastuzumab+Human+Studies)]

No references are currently available.

## Supplemental Information

[Disclaimers]

## NIH Support

Some studies in this chapter were supported by grants from the National Institutes of Health Intramural Research Program, the National Cancer Institute, and the Center for Cancer Research.

## References

1 Sharkey R.M., Goldenberg D.M. (2008). Novel radioimmunopharmaceuticals for cancer imaging and therapy. Curr Opin Investig Drugs.
2 Amoh Y., Katsuoka K., Hoffman R.M. (2008). Color-coded fluorescent protein imaging of angiogenesis: the AngioMouse models. Curr Pharm Des.
3 Barrett T., Koyama Y., Hama Y., Ravizzini G., Shin I.S., Jang B.S., Paik C.H., Urano Y., Choyke P.L., Kobayashi H. (2007). In vivo diagnosis of epidermal growth factor receptor expression using molecular imaging with a cocktail of optically labeled monoclonal antibodies. Clin Cancer Res.
4 Koyama Y., Hama Y., Urano Y., Nguyen D.M., Choyke P.L., Kobayashi H. (2007). Spectral fluorescence molecular imaging of lung metastases targeting HER2/neu. Clin Cancer Res.
5 Sampath L., Wang W., Sevick-Muraca E.M. (2008). Near infrared fluorescent optical imaging for nodal staging. J Biomed Opt.
6 Pierce M.C., Javier D.J., Richards-Kortum R. (2008). Optical contrast agents and imaging systems for detection and diagnosis of cancer. Int J Cancer.
7 Cai W., Chen X. (2007). Multimodality imaging of vascular endothelial growth factor and vascular endothelial growth factor receptor expression. Front Biosci.
8 Lee S., Park K., Kim K., Choi K., Kwon I.C. (2008). Activatable imaging probes with amplified fluorescent signals. Chem Commun (Camb).
9 Bremer C., Ntziachristos V., Weissleder R. (2003). Optical-based molecular imaging: contrast agents and potential medical applications. Eur Radiol.
10 Ntziachristos V., Bremer C., Weissleder R. (2003). Fluorescence imaging with near-infrared light: new technological advances that enable in vivo molecular imaging. Eur Radiol.
11 Wunderbaldinger P., Turetschek K., Bremer C. (2003). Near-infrared fluorescence imaging of lymph nodes using a new enzyme sensing activatable macromolecular optical probe. Eur Radiol.
12 Ogawa M., Regino C.A., Choyke P.L., Kobayashi H. (2009). In vivo target-specific activatable near-infrared optical labeling of humanized monoclonal antibodies. Mol Cancer Ther.
13 Ogawa M., Kosaka N., Choyke P.L., Kobayashi H. (2009). In vivo molecular imaging of cancer with a quenching near-infrared fluorescent probe using conjugates of monoclonal antibodies and indocyanine green. Cancer Res.
14 Palyi-Krekk Z., Barok M., Kovacs T., Saya H., Nagano O., Szollosi J., Nagy P. (2008). EGFR and ErbB2 are functionally coupled to CD44 and regulate shedding, internalization and motogenic effect of CD44. Cancer Lett.